# ^86^Y-DOTA-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^86^Y-DOTA-rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_
Abbreviated name: | ^86^Y-DOTA-ReCCMSH(Arg^11^)
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor, MC1R
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^86^Y
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily. However, these receptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via the MC1R.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) has been successfully coupled to the α-MSH peptide analogs for radiolabeling with a variety of radionuclides (7). ^111^In-, ^64^Cu- and 99mTc-DOTA-Re(Arg^11^)CCMSH showed favorable tumor imaging properties in mice bearing murine melanoma (11). A rhenium-cyclized α-MSH analog, Re-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (Re-CCMSH(Arg^11^)), was conjugated with DOTA. DOTA-Re-CCMSH(Arg^11^) was radiolabeled with ^86^Y as a potential molecular imaging agent to target melanoma (12). ^86^Y is a positron emitter with a physical t_½_ of 14.7 h and is suitable for PET imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+and+synthesis)]

McQuade et al. (12) reported the synthesis of ^86^Y-DOTA-ReCCMSH(Arg^11^).The DOTA-CCMSH(Arg^11^) peptide was synthesized using standard Fmoc/HBTU(2-[1H-benzotriazole-1-yl]-l,1,3,3,-tetramethyluroium hexafluorophosphate) chemistry on an amide resin with a peptide synthesizer as reported previously by Chen et al. (10). A mixture of DOTA-CCMSH(Arg^11^) and ReOCl_3_ (1:1.5 molar ratio) was incubated at 85°C for 30 min. The cyclized peptide, DOTA-ReCCMSH(Arg^11^), was purified by high-performance liquid chromatography (HPLC). For ^86^Y labeling, a solution of ^86^Y and DOTA-ReCCMSH(Arg^11^) was heated for 30 min at 85ºC. A radiochemical purity (as confirmed by HPLC) was >98% with specific activity of 0.23 GBq/nmol (6.2 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+in+vitro)]

Chen et al. (10) determined the 50% inhibiton concentration IC_50_ value of DOTA-ReCCMSH to be 1.2 ± 0.3 nM using B16/F1 murine melanoma cells. In comparison, the IC_50_ value of ReCCMSH was 2.9 ± 0.3 nM. Wei et al. (12) found that the IC_50_ value was 6.9 nM for Cu-DOTA-ReCCMSH.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+rodentia)]

McQuade et al. (12) performed biodistribution studies in female C57BL/6 mice (n = 5/group) bearing 10-day old B16/F1 murine melanoma tumors. Each mouse received 0.2 MBq (0.005 mCi, 0.8 pmol) ^86^Y-DOTA-ReCCMSH(Arg^11^). The radioactivity levels in percent injected dose per gram (% ID/g) were obtained at 30 min, 2 h, 4 h and 24 h after injection with tumor uptake of 11.87 ± 3.31% ID/g, 9.83 ± 2.27%ID/g, 9.98 ± 2.05% ID/g, and 0.78 ± 0.27%ID/g, respectively. The tumor retention was high up to 4 h after injection. Pre-administration of 10 nmol of DOTA-ReCCMSH(Arg^11^) significantly reduced the tumor uptake to 0.53 ± 0.31% ID/g (P <.0005) at 2 h after injection. No other tissues showed significant inhibition by DOTA-ReCCMSH(Arg^11^). The nontarget tissue (except the kidney) uptake of ^86^Y-DOTA-ReCCMSH(Arg^11^) was low at 30 min. Furthermore, the radioactivity was quickly cleared from most of the tissues (except the kidney) at 2 h after injection [e.g., kidney: 21.21 ± 4.18% ID/g at 30 min and 18.63 ± 3.62% ID/g at 2 h; liver: 0.66 ± 0.09% ID/g at 30 min and 0.28 ± 0.04% ID/g at 2 h; blood: 1.69 ± 0.28% ID/g at 30 min and 0.08 ± 0.01% ID/g at 2 h; lung: 1.81 ± 0.44% ID/g at 30 min and 0.20 ± 0.01% ID/g at 2 h;]. The tumor/muscle and tumor/blood ratios were 123 and 164 at 2 h, respectively. PET imaging of mice bearing the B16F1 melanoma was conducted with i.v. injection of 7.4 MBq (0.2 mCi, 0.034 nmol) ^86^Y-DOTA-ReCCMSH(Arg^11^) at 0.5, 2, 4 and 24 h. The tumor was clearly visible for all time point. Preinjection of 10 nmol of DOTA-ReCCMSH(Arg^11^) inhibited the tumor accumulation of radioactivity by ~80% at 0.5, 2 and 4 h after injection, whereas there was little inhibition on the kidney and liver radioactivity levels. In comparison with ^64^Cu-DOTA-ReCCMSH(Arg^11^), ^86^Y-DOTA-ReCCMSH(Arg^11^) exhibited lower nontargeted tissue radioactivity levels with the exception of the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ReCCMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=reCCMSH+AND+human)]

No publication is currently available.

## NIH Support

R24 CA86307, P50 CA103130, R24 CA86060, P30 CA91842

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Miao Y., Benwell K., Quinn T.P. (2007). 99mTc- and 111In-labeled alpha-melanocyte-stimulating hormone peptides as imaging probes for primary and pulmonary metastatic melanoma detection. J Nucl Med.
12 McQuade P., Miao Y., Yoo J., Quinn T.P., Welch M.J., Lewis J.S. (2005). Imaging of melanoma using 64Cu- and 86Y-DOTA-ReCCMSH(Arg11), a cyclized peptide analogue of alpha-MSH. J Med Chem.